# [^13^N]Ammonia

Chemical name: | [^13^N]Ammonia
Abbreviated name: | [^13^N]NH_3_
Synonym: | Ammonia N-13
Agent Category: | Compound
Target: | Glutamine synthetase
Target Category: | Metabolic trapping in cells by enzymatic conversion to [^13^N]glutamic acid
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^13^N
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nitrogen-13%20ammonia%20or%20N-13%20ammonia%20or%20%5B13N%5Dammonia)]

[^13^N]Ammonia ([^13^N]NH_3_) is a useful ^13^N-labeled compound that has been developed as a positron emission tomography (PET) imaging agent for assessing regional blood flow in tissues (1-3). The compound is labeled with ^13^N which is a positron emitter with a physical t_½_ of 9.965 min. [^13^N]NH_3_ was approved by the United States Food and Drug Administration (http://www.fda.gov/cder/regulatory/pet/default.htm) in 2000 for PET imaging of the myocardium under rest or pharmacologic stress conditions to evaluate myocardial perfusion in patients with suspected or existing coronary artery disease.

Ammonia is important in many metabolic activities of various organs and is involved in biochemical pathways leading to the production of amino acids, purines, and urea (4). Ammonia is produced in the body from the deamination of amino acids and the deamidation of amides (5). About 20% of urea produced in the body is converted to ammonia and carbon dioxide in the gut. Ammonia is absorbed and converted back to urea in the liver. It also plays a significant role in glutamine synthesis. Ammonia is produced from glutamine and other amino acids in the kidney. NH_3_, as a nonionic form, is freely permeable to all cell membranes (6). In an acidic environment, NH_3_ accepts a proton and exists as NH_4_^+^. With a dissociation constant (pK_a_) of 9.3, NH_4_^+^ constitutes about 99% of the total ammonia (NH_3_ + NH_4_^+^) concentration in the pH range of body fluids. As an ionized form, NH_4_^+^ is a relatively impermeable cation to cell membranes. The mechanism of cellular localization of [^13^N]NH_3_ is not entirely known. One known mechanism is cellular membrane diffusion of [^13^N]NH_3_ and then metabolic trapping of radioactivity with the conversion of ammonia to glutamine, glutamic acid and carbamyl phosphate (6-8).

Ammonia labeled with ^13^N was first produced by Joliot and Curie (9, 10). The short t_½_ of ^13^N requires on-site cyclotron production of ^13^N and a short synthesis time of [^13^N]NH_3_. After i.v. intravenous injection, [^13^N]NH_3_ rapidly clears from the circulation. It is taken up mainly by the myocardium, brain, liver, kidneys, and skeletal muscle (2, 6, 11, 12). In the myocardium and brain, [^13^N]NH_3_ is removed from the blood and metabolically trapped within the tissues. The apparent linear relationship between distribution of [^13^N]NH_3_ and the regional blood perfusion makes feasible the use of this radiotracer for imaging and measuring cerebral and myocardial blood flows.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20synthesis)]

As early as 1934, Joliot and Curie (10) first produced [^13^N]NH_3_ by alpha particle irradiation and heating of boron nitride in sodium hydroxide. Later, [^13^N]NH_3_ was produced by deuteron irradiation of methane gas or metal carbides, which gave relatively low yields (4). A more efficient method is the proton irradiation of a natural water target [^16^O(p,α)^13^N] (1, 13). In this procedure, [^13^N]NH_3_ is initially produced by hydrogen abstraction from the target water matrix. There is increasing production of oxo anions of nitrogen (^13^NO_3_− and ^13^NO_2_−) from radiolytic oxidation with increasing target dose. These oxo anions can be converted to [^13^N]NH_3_ in aqueous solution by use of reducing reagents such as DeVarda’s alloy in sodium hydroxide or titanium(III) chloride/hydroxide_._ Ido et al. (14) first described a fully automated synthesis method with titanium(III) chloride used as the reducing agent. The radiochemical purity was >99.9% and the radiochemical yield was 87-91% within 10 min from the end of bombardment (EOB). [^13^N]NH_3_ also can be produced directly in the target water (in-target production) by adding free radical scavengers (ethanol, acetic acid, or hydrogen) to prevent the formation of the oxo anions. Wieland et al. (15) applied this method for [^13^N]NH_3_ production with the use of pressurized, dilute aqueous solutions of acetic acid and ethanol. Berridge et al. (16) reported that the combination of hydrogen and ethanol was more effective than either alone at high beam doses. One limiting factor of the [^16^O(p,α)^13^N] nuclear reaction is that the relatively small cross-section of the reaction requires accelerators/ cyclotrons of energies >10 MeV for production.

Ferrieri et al. (17) introduced a novel solid ^13^C-enriched target for on-line [^13^N]NH_3_ production with use of the ^13^C(p,n)^13^N reaction. This nuclear reaction has a higher cross-section which can be used in accelerators/cyclotrons with <10 MeV energies. In their method, [^13^N]nitrogen gas was converted to [^13^N]NH_3_ by use of microwave radiation to dissociate the nitrogen gas in a hydrogen plasma. The reaction time was about 10 min, and radiochemical yield was 25% at 10 min after the EOB. Bida et al. (18) also used the method of ^13^C(p,n)^13^N reaction by placing enriched ^13^C carbon powder between two frits and irradiating with a 10 MeV proton beam while water was pumped through the bed to extract the ammonia. Welch et al. (19) successfully produced [^13^N]NH_3_ with the use of ^12^C(d,n)^13^N reaction and a 7 MeV deuteron beam in aluminum carbide. Shefer et al. (20) and Dence et al. (21) showed that a windowless, solid target could be irradiated with relatively low-energy (0.8-3.2 MeV) deuterons to produce [^13^N]NH_3_ by the ^12^C(d,n)^13^N reaction. This was accomplished by heating a graphite target in a stream of pure oxygen at 800ºC, and ^13^NO_2_− (99% radioactivity produced) was eluted with water and converted to [^13^N]NH_3_ with Raney nickel. The total extraction, trapping, and synthesis time was <17 min with a radiochemical purity of nearly 100%.

Mulholland et al. (22) reported a method of direct simultaneous production of [^13^N]NH_3_ and [^15^O]H_2_O with the use of 26 MeV proton irradiation and a double liquid chamber. Suzuki et al. (23) designed an automated system that used10 mM ethanol solution saturated with pure O_2_ gas as the target and bombardedment with 18 MeV protons. Krasikova et al. (24) reported an alternative method that used low-pressure methane gas (150-550 kPa) in the natural water target irradiated with protons. The radiochemical purity of [^13^N]NH_3_ was >99% even at very high beam currents. Firouzbakht et al. (25) used a cryogenic target containing frozen water for the ^16^O(p,α)^13^N reaction, and they found that this procedure (with beam currents from 1 µA to 20 µA) could produce [^13^N]NH_3_ directly because low temperature decreased radiolysis. The radiochemical purity of the [^13^N]NH_3_ produced was >95%. When frozen carbon dioxide was irradiated, >95% of ^13^N activity was in the form of nitrate and nitrite.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20in%20vitro)]

Isolated arterially perfused rabbit interventricular septa (n = 9 at 28ºC, n = 10 at 37ºC) were used to study the relationship between blood flow, myocardial uptake, and the metabolism and clearance of [^13^N]NH_3_ (8). Analysis of the time-activity curves revealed that the [^13^N]NH_3_ kinetics were best described by three components. Component 1, with a short clearance t_½_ of <7 min, was consistent with a freely diffusible NH_3_ compartment. A large metabolic compartment was primarily responsible for component 3, which had a long clearance t_½_ of 30 to 500 min. At 37^o^C and 15 min after injection, all radioactivity was essentially in component 3. In another study, glutamine synthetase appeared to be responsible for retention of [^13^N]NH_3_ radioactivity in rabbit myocardium (26). In their study of [^13^N]NH_3_ uptake in myocardial single cells, Rauch et al. (27) found that in addition to metabolic trapping, the extraction of [^13^N]NH_3_ might also be influenced by cell membrane integrity, intracellular-extracellular pH gradient, and possibly an anion exchange system for bicarbonate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28N-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20rodentia)]

Imaging studies with [^13^N]NH_3_ in mice showed activity localization in the liver, myocardium, and bladder (12). The radioactivity cleared from the blood very rapidly with 85% clearance in the first minute, and 4.7% of the injected dose (ID) was excreted by the kidneys in 35 min. The biodistribution of [^13^N]NH_3_ was studied in rats (28). The rats were euthanized at different time intervals between 0.2 and 50 min after i.v. injection of 18.5 MBq (0.5 mCi)/kg of [^13^N]NH_3_ with an estimated specific activity of 74 × 10^5^ to 148 × 10^5^ GBq/mol (2 × 10^5^ to 4 × 10^5^ Ci/mol) at the EOB. The highest initial whole-organ radioactivities at 0.2 min after injection were in the lungs (20.1 ± 2.9% ID n = 5), kidneys (13.6 ± 1.2% ID), and heart (2.6 ± 0.18% ID), and at 50 min these values decreased to 1.51 ± 0.17% ID, 1.82 ± 0.22% ID, and 0.92 ± 0.06% ID, respectively. The radioactivity in the liver was 4.83 ± 0.73% ID at 0.2 min and then increased to a maximum of 14.4 ± 0.7% ID at 20 min. The radioactivity in the brain was 0.55 ± 0.04% ID at 0.2 min and then increased to a maximum of 0.89 ± 0.1% ID at 10 min.

Cooper et al. (29) studied the cerebral uptake and metabolism of [^13^N]NH_3_ in conscious rats, and they found that [^13^N]NH_3_ entered the brain from the blood largely by diffusion. This and other studies (30) indicated that the major route for metabolism of [^13^N]NH_3_ in the brain was incorporation into [amide-^13^N]glutamine. Lockwood et al. (31) showed that the brain-blood pH gradient had a major influence on the uptake of [^13^N]NH_3_ by the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The localization of [^13^N]NH_3_ was studied in normal dogs by three methods of administration (inhalation, i.v., and s.c.) (4). All three methods showed similar imaging results. The radioactivity localization was mainly in the brain, heart, liver, and bladder. Approximately 10-20% of the ID was cleared rapidly from the blood by the kidneys and collected in the urinary bladder. The clearance t_½_ of the kidneys was 7.7 to 10.6 min. In a dog study, Carter et al. (32) showed that increased blood pH increased brain uptake of [^13^N]NH_3_ and decreased blood pH decreased liver uptake of [^13^N]NH_3_. Rosenspire et al. (33) studied the metabolic fate of [^13^N]NH_3_ in dogs, and they found that urea was the predominant metabolite. Neutral amino acids (i.e., glutamine and asparagine) were the second most predominant metabolites. Schelbert et al. (34, 35) found a relatively linear relationship between myocardial blood flow (from 0 to 500 ml/min/100 g in dogs) and myocardial [^13^N]NH_3_ radioactivity concentration. In comparison, the human physiologic range was from 0 to 350 ml/min/100 g. Other studies in dogs (36, 37) indicated that [^13^N]NH_3_ provided qualitative and quantitative information of myocardial blood flow comparable to data measured by microspheres and [^15^O]H_2_O.

The uptake kinetics of [^13^N]NH_3_ in the liver were studied in a pig model (38). A simplified circulatory model was proposed to estimate the hepatic clearance of [^13^N]NH_3_. The hepatic clearance was estimated to be 10.25 ± 1.84 ml/min/kg (n = 4).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20%28primate%20NOT%20human%29)]

The movement of [^13^N]NH_3_ from blood to brain was studied in rhesus monkeys (39). A regional residue detection model was proposed for the cerebral blood flow. The data revealed a diffusion limitation for the transport of [^13^N]NH_3_ from blood to brain because of the low permeability of [^13^N]NH_4_^+^.Therefore at high flow rates the brain uptake of [^13^N]NH_3_ was no longer linear with flow increases.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%20AND%20human)]

Harper et al. (12) performed imaging with 370 MBq (10 mCi) at the time of administration, (TOA) of [^13^N]NH_3_ in 2 healthy volunteers and showed that radioactivity localized in the myocardium, mediastinum, and liver. There was an initial moderate uptake in the lungs, and it was washed out after 5-10 min. In a metabolic study (33), 9 healthy male volunteers received iv. administration of 740 MBq (20 mCi at the TOA) of [^13^N]NH_3_ in normal saline. About 93.1 ± 4.9% (n = 6) of the blood radioactivity remained as [^13^N]NH_3_ within the first 2 min but was decreased to 50.2 ± 18.9% (n = 5) at 5 min after injection. At 1 min, the blood radioactivities associated with [^13^N]glutamine and [^13^N]urea were 3.0 ± 2.4% (n = 6) and 3.1 ± 4.6%, respectively. By 5 min, the radioactivities for [^13^N]glutamine and [^13^N]urea had increased to 16.2 ± 11.2% (n = 5) and 32.7 ± 10.0%, respectively. Lockwood et al. (11) reported a study of [^13^N]NH_3_ metabolism in 5 normal subjects with a dose of 370 MBq (10 mCi at the TOA) that showed that the rates of both radioactivity clearance from the vascular compartment and brain ammonia utilization were linear functions of its arterial concentration. About 47 ± 3% of [^13^N]NH_3_ radioactivity was taken up by the brain during a single pass from the arterial blood, and 7.4 ± 0.3% of [^13^N]NH_3_ was metabolized by the brain. Approximately 50% of the arterial [^13^N]NH_3_ was metabolized by the skeletal muscle. Changes in [^13^N]NH_3_ kinetics were reported in patients with tumors, hypopituitarism, and liver diseases [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%29%20AND%20%28hypopituitarism%20or%20tumor%20or%20liver%20disease%29)].

In 1980, Lockwood (40) reported the radiation absorbed doses of i.v. injection of [^13^N]NH_3_ with the use of body distribution data and the MIRD model. The urinary bladder wall was the critical organ with the highest total absorbed dose (0.014 mGy/MBq or 51 mrad/mCi). The whole body, liver, red marrow, ovaries, and testes received 0.0015 mGy/MBq (5.5 mrad/mCi), 0.0046 mGy/MBq (17 mrad/mCi), 0.0015 mGy/MBq (5.4 mrad/mCi), 0.0027 mGy/MBq (9.8 mrad/mCi), and 0.00027 mGy/Bq (1 mrad/mCi), respectively. The brain to brain-absorbed dose was 0.0043 mGy/MBq (16 mrad/mCi). Complete radiation dosimetry (http://www.internaldosimetry.com/freedosestimates/adult/linkedpages/n13amm.html) of [^13^N]NH_3_ for adults has also been tabulated.

Hickey et al. (41) in a 2005 study compared the measurement of myocardial perfusion using [^13^N]NH_3_ with that of [^15^O]H_2_O in healthy volunteers, and they found that there was a discrepancy between the two measurements in a 2-compartment model analysis. The underestimation by [^13^N]NH_3_ was most likely attributable to the regional myocardial uptake variation and metabolism of [^13^N]NH_3_. This could be minimized by use of a 3-compartment model for data analysis. Other studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28nitrogen-13%20ammonia%20or%2013N-ammonia%20or%20%5B13N%5Dammonia%20AND%20myocardial%20study)] have shown the clinical utility of [^13^N]NH_3_ for quantification of myocardial blood flow in humans. In a study of 27 patients, Khorsand et al. (42) reported that gated cardiac [^13^N]NH_3_ imaging could be used for the estimation of LV function. In a study of 21 patients admitted for the assessment of myocardial perfusion with dynamic [^13^N]NH_3_ PET, the absolute quantification of myocardial blood flow with 3-dimensional PET appeared to be in excellent agreement with those obtained with the 2-dimensional technique (43).

## Supplemental Information

[Disclaimers]

Draft of Review and Evaluation of Pharmacology and Toxicology Data

Medical and Statistical Review

## NIH Support

NIH HL-27841-01-03; NCI CA-18153-03, CA-08748-14; USPHS AM-16739, NS-00343; NIH DK-16739; NINCDS NS-05820, NS15665; NIH HL-11351-13, HL-27841-01; NCI 08748-11B; NIH RO1 HL-41047-01; USPHS GM-14889-06, 1 F11 NB-2169-01; NIH HL-29845, HL-33177, HL-29845-01; USPHS HE-06664, HL-15860, GM-16712, HV-71443; NCI CA-08748; NIH HL-43884; NINDS NS-15380; PHS NINCDS NS-15380; USPHS P01 HL-13851-11; NIH IR43HL48969, 2R44CA53953; NIH NS15655; NIH NS-02149; USPHS 1 P01 GM-18940-01, 43-NHL1-68-1334; NINCDS NS-05820, NS-14996, NIH 89-2359Ja, HL-27555, NIH HL-29845, HL-33177.

## References

1. Clark, J.C., F.I. Aigbirdhio, Chemistry of nitrogen-13 and oxygen-15, in Handbook of Radiopharmaceuticals, M.J. Welch, C.S. Redvanly, Editor. 2003, John Wiley & Sons Inc.: Chichester, West Sussex, England. p. 119-140.
2 Phelps M.E., Hoffman E.J., Raybaud C. (1977). Factors which affect cerebral uptake and retention of 13NH3. Stroke.
3. Schelbert, H.R., PET studies of the heart., in Positron Emission Tomography and Autoradiography, M.E. Phelps, J.C. Mazziota and H.R. Schelbert, Editor. 1986, Raven Press: New York. p. 581-662.
4 Monahan W.G., Tilbury R.S., Laughlin J.S. (1972). Uptake of 13 N-labeled ammonia. J Nucl Med.
5. Mudge, G.H., Agents affecting volume and composition of body fluids, in Goodman and Gilman's the pharmacological basis of therapeutics, A.G. Gilman, L.S. Goodman and A. Gilman, Editor. 1980, MacMillan Publishing Co., Inc.: New York. p. 869-870.
6 Walsh W.F., Fill H.R., Harper P.V. (1977). Nitrogen-13-labeled ammonia for myocardial imaging. Semin Nucl Med.
7 Straatmann M.G. (1977). A look at 13N and 15O in radiopharmaceuticals. Int J Appl Radiat Isot.
8 Krivokapich J., Huang S.C., Phelps M.E., MacDonald N.S., Shine K.I. (1982). Dependence of 13NH3 myocardial extraction and clearance on flow and metabolism. Am J Physiol.
9 Schelstraete K., Simons M., Deman J., Vermeulen F.L., Slegers G., Vandecasteele C., Goethals P., De Schryver A. (1982). Uptake of 13N-ammonia by human tumours as studied by positron emission tomography. Br J Radiol.
10 Joliot F., Curie I. (1934). Artifical production of a new kind of radio-element. Nature.
11 Lockwood A.H., McDonald J.M., Reiman R.E., Gelbard A.S., Laughlin J.S., Duffy T.E., Plum F. (1979). The dynamics of ammonia metabolism in man. Effects of liver disease and hyperammonemia. J Clin Invest.
12 Harper P.V., Lathrop K.A., Krizek H., Lembares N., Stark V., Hoffer P.B. (1972). Clinical feasibility of myocardial imaging with 13 NH 3. J Nucl Med.
13 van den Heuvel A.F., Blanksma P.K., Siebelink H.M., van Wijk L.M., Boomsma F., Vaalburg W., Crijns H.J., van Veldhuisen D.J. (2001). Impairment of myocardial blood flow reserve in patients with asymptomatic left ventricular dysfunction: effects of ACE-inhibition with perindopril. Int J Cardiovasc Imaging.
14 Ido T., Iwata R. (1981). Fully automated synthesis of 13NH3. Journal of Labelled Compounds and Radiopharmaceuticals.
15 Wieland B., Bida G., Padgett H., Hendry G., Zippi E., Kabalka G., Morelle J.L., Verbruggen R., Ghyoot M. (1991). In-target production of [13N]ammonia via proton irradiation of dilute aqueous ethanol and acetic acid mixtures. Int J Rad Appl Instrum [A].
16 Berridge M.S., Landmeier B.J. (1993). In-target production of [13N]ammonia: target design, products, and operating parameters. Appl Radiat Isot.
17 Ferrieri R.A., Schlyer D.J., Wieland B.W., Wolf A.P. (1983). On-line production of 13N-nitrogen gas from a solid enriched 13C-target and its application to 13N-ammonia synthesis using microwave radiation. Int. J. Appl. Radiat. Isot.
18 Bida G., Wieland B. W., Ruth T.J., Schmidt D.G., Hendry G.O., Keen R.E. (1986). An economical target for nitrogen-13 production by proton bombardment of a slurry of C-13 powder in O-16 water. J. Labelled Compd. Radiopharm.
19 Welch M.J., Lifton J.F. (1971). The fate of nitrogen-13 formed by the 12C(d,n)13N reaction in inorganic carbides. Journal of the American Chemical Society.
20 Shefer R.E., Hughey B.J., Klinkowstein R.E., Welch M.J., Dence C.S. (1994). A windowless 13N production target for use with low energy deuteron accelerators. Nucl Med Biol.
21 Dence C.S., Welch M.J., Hughey B.J., Shefer R.E., Klinkowstein R.E. (1994). Production of [13N]ammonia applicable to low energy accelerators. Nucl Med Biol.
22 Mulholland G.K., Kilbourn M.R., Moskwa J.J. (1990). Direct simultaneous production of [15O]water and [13N]ammonia or [18F]fluoride ion by 26 MeV proton irradiation of a double chamber water target. Int J Rad Appl Instrum [A].
23 Suzuki K., Yoshida Y., Shikano N., Kubodera A. (1999). and Development of an automated system for the quick production of 13N-labeled compounds with high specific activity using anhydrous [13N]NH3. Applied Radiation adn Isotopes, 50: p. 1033-1038.
24 Krasikova R.N., Fedorova O.S., Korsakov M.V., Bennington B.I., Berridge M.S. (1999). Improved [N-13]ammonia yield from the proton irradiation of water using methane gas. Appl. Radiat. Isot.
25 Firouzbakht M.L., Schlyer D.J., Wolf A.P., Fowler J.S. (1999). Mechanism of nitrogen-13-labeled ammonia formation in a cryogenic water target. Nucl Med Biol.
26 Krivokapich J., Barrio J.R., Phelps M.E., Watanabe C.R., Keen R.E., Padgett H.C., Douglas A., Shine K.I. (1984). Kinetic characterization of 13NH3 and [13N]glutamine metabolism in rabbit heart. Am J Physiol.
27 Rauch B., Helus F., Grunze M., Braunwell E., Mall G., Hasselbach W., Kubler W. (1985). Kinetics of 13N-ammonia uptake in myocardial single cells indicating potential limitations in its applicability as a marker of myocardial blood flow. Circulation.
28 Freed B.R., McQuinn R.L., Tilbury R.S., Digenis G.A. (1982). Distribution of 13N in rat tissues following intravenous administration of nitroso-labeled BCNU. Cancer Chemother Pharmacol.
29 Cooper A.J., McDonald J.M., Gelbard A.S., Gledhill R.F., Duffy T.E. (1979). The metabolic fate of 13N-labeled ammonia in rat brain. J Biol Chem.
30 Cooper A.J., Lai J.C. (1987). Cerebral ammonia metabolism in normal and hyperammonemic rats. Neurochem Pathol.
31 Lockwood A.H., Finn R.D., Campbell J.A., Richman T.B. (1980). Factors that affect the uptake of ammonia by the brain: the blood-brain pH gradient. Brain Res.
32 Carter C.C., Lifton J.F., Welch M.J. (1973). Organ uptake and blood pH and concentration effects of ammonia in dogs determined with ammonia labeled with 10 minute half-lived nitrogen 13. Neurology.
33 Rosenspire K.C., Schwaiger M., Mangner T.J., Hutchins G.D., Sutorik A., Kuhl D.E. (1990). Metabolic fate of [13N]ammonia in human and canine blood. J Nucl Med.
34 Schelbert H.R., Phelps M.E., Hoffman E.J., Huang S.C., Selin C.E., Kuhl D.E. (1979). Regional myocardial perfusion assessed with N-13 labeled ammonia and positron emission computerized axial tomography. Am J Cardiol.
35 Schelbert H.R., Phelps M.E., Huang S.C., MacDonald N.S., Hansen H., Selin C., Kuhl D.E. (1981). N-13 ammonia as an indicator of myocardial blood flow. Circulation.
36 Muzik O., Duvernoy C., Beanlands R.S., Sawada S., Dayanikli F., Wolfe E.R., Schwaiger M. (1998). Assessment of diagnostic performance of quantitative flow measurements in normal subjects and patients with angiographically documented coronary artery disease by means of nitrogen-13 ammonia and positron emission tomography. J Am Coll Cardiol.
37 Bol A., Melin J.A., Vanoverschelde J.L., Baudhuin T., Vogelaers D., De Pauw M., Michel C., Luxen A., Labar D., Cogneau M., Robert A., Heyndrickx G., Wijns W. (1993). Direct comparison of [13N]ammonia and [15O]water estimates of perfusion with quantification of regional myocardial blood flow by microspheres. Circulation.
38 Weiss M., Roelsgaard K., Bender D., Keiding S. (2002). Determinants of [13N]ammonia kinetics in hepatic PET experiments: a minimal recirculatory model. Eur J Nucl Med Mol Imaging.
39 Raichle M.E., Larson K.B. (1981). The significance of the NH3-NH+(4) equilibrium on the passage of 13N-ammonia from blood to brain. A new regional residue detection model. Circ Res.
40 Lockwood A.H. (1980). Absorbed doses of radiation after an intravenous injection of N-13 ammonia in man: concise communication. J Nucl Med.
41 Hickey K.T., Sciacca R.R., Chou R.L., Rodriguez O., Bokhari S., Bergmann S.R. (2005). An improved model for the measurement of myocardial perfusion in human beings using N-13 ammonia. J Nucl Cardiol.
42 Khorsand A., Graf S., Eidherr H., Wadsak W., Kletter K., Sochor H., Schuster E., Porenta G. (2005). Gated Cardiac 13N-NH3 PET for Assessment of Left Ventricular Volumes, Mass, and Ejection Fraction: Comparison with Electrocardiography-Gated 18F-FDG PET. J Nucl Med.
43 Schepis T., Gaemperli O., Treyer V., Valenta I., Burger C., Koepfli P., Namdar M., Adachi I., Alkadhi H., Kaufmann P.A. (2007). Absolute quantification of myocardial blood flow with 13N-ammonia and 3-dimensional PET. J Nucl Med.